# N-4'-[^18^F]Fluorobenzylpiperidin-4yl-(2-fluorophenyl)acetamide

Chemical name: | N-4'-[^18^F]Fluorobenzylpiperidin-4yl-(2-fluorophenyl)acetamide
Abbreviated name:
Synonym: | [^18^F]FBFPA
Agent Category: | Compound
Target: | σ_1_ sigma receptors
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FBFPA)]

Sigma receptors are functional membrane-bound proteins distributed in the central nervous system (CNS) and peripheral organs such as the liver, kidneys, and endocrine glands (1, 2). The CNS sigma receptors are unique binding sites related to higher brain function. There are at least two subtypes of sigma receptors, σ_1_ and σ_2_. These receptors appear to be involved in numerous pharmacologic and physiologic functions, and they also modulate a number of central neurotransmitter systems. Studies suggest that these receptors may play a role in the pathogenesis of psychiatric disorders (3, 4). The σ_1_ receptors appear to play a role in CNS disorders and motor functions. The σ_2_ receptors, which are linked to potassium channels and calcium release, are also implicated in malignant neoplastic diseases (5-7). The density of σ_2_ receptors in tumor cells was found to be greater than that of σ_1_ receptors. For example, the density of σ_2_ receptors was found to be 10-fold higher in proliferating versus quiescent mouse mammary adenocarcinoma cells. Furthermore, it has been observed that σ_2_ receptor ligands can induce apoptosis in tumor cells. Because of these effects, sigma receptor ligands may be useful for detection and treatment in neurology and oncology.

Matsuno et al. (8) have developed a potent σ_1_ agonist, 1-(3,4-dimethoxyphenethyl)-4-(3-phenylpropyl)-piperazine dihydrochloride (SA4503), which exhibits a 14-fold selectivity for σ_1_ receptors over σ_2_ receptors.SA4503 has been labeled with ^11^C and ^18^F for positron emission tomography (PET) studies of sigma receptors in monkeys and humans (3, 9-11). Huang et al. (12) have reported a series of N-benzylpiperidin-4yl-phenylacetamide analogs with high affinity for σ_1_ receptors and relatively low affinity for σ_2_ receptors. One of these analogs has been radiolabeled as N-4'-[^18^F]fluorobenzylpiperidin-4yl-(2-fluorophenyl)acetamide ([^18^F]FBFPA) for PET imaging of CNS σ_1_ receptors (13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FBFPA%20and%20synthesis)]

[^18^F]FBFPA was synthesized by N-alkylation of the desbenzyl compound piperidin-4yl-(2-fluorophenyl)acetamide with [^18^F]4’-fluorobenzyliodide in dimethyformamide at 90°C for 10 min (13). After chromatographic separation, the overall yield of [^18^F]FBFPA was 20% based on [^18^F]CsF. The specific activity was 37–74 GBq/μmol (1–2 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FBFPA%20and%20in%20vitro)]

FBFPA has been reported by Huang et al. (12) to have selective binding affinity to σ_1_ receptor sites in homogenates of guinea pig brain membranes versus σ_2_ binding sites in rat liver membranes. The inhibition constant (K_i_) values for σ_1_ and σ_2_ were 3.15 ± 0.05 and 139.51 ± 21.89 nM, respectively. Therefore, FBFPA exhibited a 44-fold selectivity for σ_1_ receptors over σ_2_ receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FBFPA%20and%20rodentia)]

Mach et al. (13) performed brain biodistribution studies in normal rats. Their studies showed there was 0.87% injected dose (ID)/g in the whole brain at 5 min after injection of [^18^F]FBFPA, with gradual washout to 0.53% ID/g at 120 min. On the other hand, there was rapid washout of radioactivity from the blood, which resulted in brain/blood ratios of 15 at 5 min and 53 at 120 min. There was a high accumulation and progressive washout of radioactivity in the frontal cortex, striatum, hippocampus, and cerebellum. Co-injection of [^18^F]FBFPA with 1 mg/kg unlabeled FBFPA inhibited uptake to all the brain regions by >80%. Pretreatment with 40 mg/kg progesterone, a putative endogenous ligand, 30 min before tracer injection reduced the brain uptake by ~50%.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FBFPA%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FBFPA%20and%20%28primate%20not%20human%29)]

Biodistribution PET studies in rhesus monkeys injected with 207.2–229.4 MBq (5.6–6.2 mCi) [^18^F]FBFPA were performed by Mach et al. (13) and showed rapid accumulation of radioactivity in the brain. PET study showed selective maximal uptake in the regions of the cingulate cortex, followed by the temporal cortex, parietal cortex, and occipital cortex. The cerebellum showed lower binding than the other brain regions. The peak level in the brain (0.045% ID/ml) was reached in the cingulated cortex at 10 min, followed by gradual washout to ~0.025% ID/ml at 180 min. Injection of 1 mg/kg haloperidol, a σ_1_/ σ_2_ ligand, 40 min after injection of [^18^F]FBFPA dramatically decreased radioactivity in the brain regions studied.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FBFPA%20and%20human)]

No publication is currently available.

## NIH Support

CA818025-01

## References

1 Bowen W.D. (2000). Sigma receptors: recent advances and new clinical potentials. Pharm Acta Helv.
2 Walker J.M., Bowen W.D., Walker F.O., Matsumoto R.R., De Costa B., Rice K.C. (1990). Sigma receptors: biology and function. Pharmacol Rev.
3 Mishina M., Ishiwata K., Ishii K., Kitamura S., Kimura Y., Kawamura K., Oda K., Sasaki T., Sakayori O., Hamamoto M., Kobayashi S., Katayama Y. (2005). Function of sigma1 receptors in Parkinson's disease. Acta Neurol Scand.
4 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
5 Colabufo N.A., Berardi F., Contino M., Ferorelli S., Niso M., Perrone R., Pagliarulo A., Saponaro P., Pagliarulo V. (2006). Correlation between sigma2 receptor protein expression and histopathologic grade in human bladder cancer. Cancer Lett.
6 Vilner B.J., John C.S., Bowen W.D. (1995). Sigma-1 and sigma-2 receptors are expressed in a wide variety of human and rodent tumor cell lines. Cancer Res.
7 Wheeler K.T., Wang L.M., Wallen C.A., Childers S.R., Cline J.M., Keng P.C., Mach R.H. (2000). Sigma-2 receptors as a biomarker of proliferation in solid tumours. Br J Cancer.
8 Matsuno K., Nakazawa M., Okamoto K., Kawashima Y., Mita S. (1996). Binding properties of SA4503, a novel and selective sigma 1 receptor agonist. Eur J Pharmacol.
9 Elsinga P.H., Tsukada H., Harada N., Kakiuchi T., Kawamura K., Vaalburg W., Kimura Y., Kobayashi T., Ishiwata K. (2004). Evaluation of [18F]fluorinated sigma receptor ligands in the conscious monkey brain. Synapse.
10 Ishiwata K., Tsukada H., Kawamura K., Kimura Y., Nishiyama S., Kobayashi T., Matsuno K., Senda M. (2001). Mapping of CNS sigma(1) receptors in the conscious monkey: preliminary PET study with [(11)C]SA4503. Synapse.
11 van Waarde A., Buursma A.R., Hospers G.A., Kawamura K., Kobayashi T., Ishii K., Oda K., Ishiwata K., Vaalburg W., Elsinga P.H. (2004). Tumor imaging with 2 sigma-receptor ligands, 18F-FE-SA5845 and 11C-SA4503: a feasibility study. J Nucl Med.
12 Huang Y., Hammond P.S., Wu L., Mach R.H. (2001). Synthesis and structure-activity relationships of N-(1-benzylpiperidin-4-yl)arylacetamide analogues as potent sigma1 receptor ligands. J Med Chem.
13 Mach R.H., Gage H.D., Buchheimer N., Huang Y., Kuhner R., Wu L., Morton T.E., Ehrenkaufer R.L. (2005). N-[18F]4'-fluorobenzylpiperidin-4yl-(2-fluorophenyl) acetamide ([18F]FBFPA): a potential fluorine-18 labeled PET radiotracer for imaging sigma-1 receptors in the CNS. Synapse.